# ^99m^Tc-glutamate peptide 3-aminoethyl estradiol

Chemical name: | ^99m^Tc-Glutamate peptide-3-aminoethyl estradiol | [image]
Abbreviated name: | ^99m^Tc-GAP-EDL | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Estrogen receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging | [image]
Source of signal/contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | The exact location of ^99m^Tc in the structure of ^99m^Tc-GAP-EDL is unknown.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL)]

A favorable prognosis of estrogen therapy for breast cancer can often be predicted on the basis of response to the hormone because the estrogen receptor (ER) is a valuable marker to determine treatment outcome (1). The ER status of the tumors determines the likelihood of a favorable response to the treatment, and patients with ER-positive tumors have a better chance of recovery compared to those with ER-negative tumors. The presence of ER in the tissue is measured in a biopsy sample or after resection of a tumor. The random biopsy or tumor sampling may yield a false negative result because primary tumors usually have a heterogeneous ER distribution (2). In this regard a radioscintigraphic procedure could be more useful to determine the ER status of tumors because agents used for scintigraphy have a binding specificity for their targets.

Tamoxifen is a selective ER modulator that blocks estrogen binding to the receptor and is often used to treat breast cancer. Using radioactive halogen ([^18^F] fluorine and [^131^I] iodine) derivatives of tamoxifen in conjunction with positron emission tomography (PET), some investigators have investigated and monitored the effects of this drug at the cellular and clinical levels for the treatment of cancer (3-6). Although the results obtained from these studies are encouraging, the expenses, availability, and water solubility of these derivatives are limiting factors for clinical use. As an alternative, Takahashi et al. decided to develop a meta-stable, technetium (^99m^Tc)-labeled derivative of estradiol (EDL) to possibly investigate and monitor ER status in cancer patients because the isotope is inexpensive and easily available, and the derivative is water-soluble (7); this estradiol was conjugated to a poly-glutamate peptide (GAP) that could chelate the ^99m^Tc isotope to obtain ^99m^Tc-GAP-EDL for imaging and radiotherapeutic purposes. The investigators also explored the possibility of using ^99m^Tc-GAP-EDL to detect endometriosis, an ER-associated condition, using a rabbit model (7-9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+synthesis)]

The synthesis of ^99m^Tc -GAP-EDL was performed as described by Takahashi et al. (7, 9). To start, estrone was dissolved in anhydrous ethanol. Sodium ethoxide and bromoacetonitrile were added to the solution and the mixture was heated under reflux for 3 h. The ethanol was allowed to evaporate completely and the residue was dissolved in ethyl acetate. The mixture was washed with water and the organic layer was filtered after drying over magnesium sulphate. The ethyl actetate was evaporated under reduced pressure and the remaining solid product, 3-acetonitrile estradiol, was washed with ether. The yield of this reaction was 75%. The solid product was dissolved in tetrahydrofuran, and lithium aluminum hydride was added to the mixture and stirred for 4 h. The solvent was evaporated to yield a solid that was dissolved in ethyl acetate. This solution was washed with water, dried over magnesium sulphate, and filtered. The solvent was evaporated to obtain 3-cyanomethyl estrone (EDL) with a yield of 92%. The structure of EDL was confirmed by nuclear magnetic resonance.

For the synthesis of GAP-EDL, the sodium salt of GAP was converted to the acid form by the addition of 2 N hydrochloric acid (HCl). This solution was dialyzed to remove all the HCl and freeze-dried to obtain the acidic form of GAP. The GAP acid was dissolved in dimethylformamide (DMF), and dicyclohexyl carbodiimide and 4-N,N-dimethyl aminopyridine were added to it. This mixture was stirred at room temperature for 2 days. The DMF was evaporated under reduced pressure; 1 N sodium bicarbonate was added to it and extracted with chloroform. The aqueous solution was dialyzed, filtered, and freeze-dried to obtain GAP-EDL. The percent yield of this reaction was not provided in the publication. The GAP-EDL complex contained 15% (weight/weight) EDL as determined by ultraviolet spectroscopy.

For the synthesis of ^99m^Tc-GAP-EDL, ^99m^Tc was added to a vial containing lyophilized GAP-EDL and tin (II) chloride. Using a radio thin-layer chromatography scanner, the radiochemical purity of the product was determined to be 97%. The Rf value and specific activity of ^99m^Tc-GAP-EDL were not provided in the publication (7). The synthesis and specific activities of ^99m^Tc-GAP and ^99m^Tc-labeled diethylenetriamene pentaacetate (DTPA), used as controls in the studies, were not presented in the publications (7, 9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+in+vitro)]

The uptakes of ^99m^Tc-GAP and ^99m^Tc-GAP-EDL were investigated in ER-positive cell lines (ie, MCF-7 (http://www.atcc.org/catalog/numSearch/numResults.cfm?atccNum=HTB-22) (of human breast adenocarcinoma origin), T-47D (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=HTB-133) (of human breast carcinoma origin), and 13762 MAT B III (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-1666) (of rat mammary adenocarcinoma origin) (7). An ER-negative cell line, RAB-9 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-1414) (of rabbit skin origin), was used as a control in the studies (9). The uptake of ^99m^Tc-GAP-EDL was significantly higher than ^99m^Tc-GAP in the MCF-7, T-47D, and 13762 MAT B III cells. Prior exposure of these cells to diethylstilbestrol (DES), a synthetic estrogen, resulted in a 70% reduction of ^99m^Tc-GAP-EDL uptake (7). In the same study, MCF-7 cells treated with tamoxifen showed a 10% decrease in uptake of the radiochemical. The rate of uptake and accumulation of ^99m^Tc-GAP-EDL was ~4-fold higher in the MCF-7 versus the RAB cells (9). On the basis of these observations, the investigators concluded that the in vitro uptake of ^99m^Tc-GAP-RDL was an ER-mediated process.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+rodentia)]

Tissue distribution studies of ^99m^Tc-GAP-EDL were performed in rats bearing 13762 MAT B III cell tumors (7). The animals (n = 3 per time point) were injected with either ^99m^Tc-GAP-EDL or ^99m^Tc-GAP and euthanized 0.5–4 h later. Selected tissues from the animals were excised, collected, and counted for incorporated radioactivity. Radioactivity levels, given as % injected dose/gram (%ID/g) for tumor/muscle increased as a function of time and were significantly higher (P<0.05) 4 h after administration for animals injected with ^99m^Tc-GAP-EDL (7.92 ± 0.56% ID/g) compared to those injected with ^99m^Tc-GAP (6.01 ± 0.05% ID/g). Similar observations were also made for the uterus/muscle and uterus/blood count ratios.

Planar scintigraphy with ^99m^Tc-GAP-EDL and ^99m^Tc-DTPA was also performed on rats bearing 13762 MAT B III cell tumors (7). In blocking studies, the rats were treated with DES 1 h before administration of ^99m^Tc-GAP-EDL. Region-of-interest analysis of the planar images 0.5 and 4 h after administration of the labels showed that the tumor/muscle ratios were 1.67–2.95 and 1.26–1.75 for ^99m^Tc-GAP-EDL and ^99m^Tc-DTPA, respectively. In the blocking study, the ratios were 1.98–2.39 and 1.21–1.63 for ^99m^Tc-GAP-EDL and the DES pre-treated animals, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+nonprimate+mammals)]

The use of ^99m^Tc-GAP-EDL for the detection of endometriosis was evaluated in a rabbit model (7, 9). An established procedure was used to induce endometriosis in the animals (10). Eight weeks after surgery, ^99m^Tc-GAP-EDL was intravenously administered to the animals, and scintigraphic images were obtained 0.5–2 h after the injection. The rabbits were then euthanized, and the grafts were excised for histological examination. In comparison to the surrounding tissue, the uterus, ovaries, and the implants showed an increased uptake of ^99m^Tc-GAP-EDL. The radiotracer was also detected in the microinvasive endometrial tissue. A microscopic examination of the tissue supported the observations made after imaging. From these observations the investigators suggest that ^99m^Tc-GAP-EDL was taken up by the tissue through an ER-mediated process. No blocking studies for ^99m^Tc-GAP-EDL uptake were reported.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+nonhuman+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+GAP+EDL+human+studies)]

No publications are currently available.

## References

1 Chen W.Y., Colditz G.A. (2007). Risk factors and hormone-receptor status: epidemiology, risk-prediction models and treatment implications for breast cancer. Nat Clin Pract Oncol.
2 van Netten J.P., Armstrong J.B., Carlyle S.S., Goodchild N.L., Thornton I.G., Brigden M.L., Coy P., Fletcher C. (1988). Estrogen receptor distribution in the peripheral, intermediate and central regions of breast cancers. Eur J Cancer Clin Oncol.
3 Inoue T., Kim E.E., Wallace S., Yang D.J., Wong F.C., Bassa P., Cherif A., Delpassand E., Buzdar A., Podoloff D.A. (1996). Positron emission tomography using [18F]fluorotamoxifen to evaluate therapeutic responses in patients with breast cancer: preliminary study. Cancer Biother Radiopharm.
4 Yang D.J., Li C., Kuang L.R., Price J.E., Buzdar A.U., Tansey W., Cherif A., Gretzer M., Kim E.E., Wallace S. (1994). Imaging, biodistribution and therapy potential of halogenated tamoxifen analogues. Life Sci.
5 Aliaga A., Rousseau J.A., Ouellette R., Cadorette J., van Lier J.E., Lecomte R., Benard F. (2004). Breast cancer models to study the expression of estrogen receptors with small animal PET imaging. Nucl Med Biol.
6 Seimbille Y., Benard F., Rousseau J., Pepin E., Aliaga A., Tessier G., van Lier J.E. (2004). Impact on estrogen receptor binding and target tissue uptake of [18F]fluorine substitution at the 16alpha-position of fulvestrant (faslodex; ICI 182,780). Nucl Med Biol.
7 Takahashi N., Yang D.J., Kohanim S., Oh C.S., Yu D.F., Azhdarinia A., Kurihara H., Zhang X., Chang J.Y., Kim E.E. (2007). Targeted functional imaging of estrogen receptors with 99mTc-GAP-EDL. Eur J Nucl Med Mol Imaging.
8 Hudelist G., Keckstein J., Czerwenka K., Lass H., Walter I., Auer M., Wieser F., Wenzl R., Kubista E., Singer C.F. (2005). Estrogen receptor beta and matrix metalloproteinase 1 are coexpressed in uterine endometrium and endometriotic lesions of patients with endometriosis. Fertil Steril.
9 Takahashi N., Yang D.J., Kurihara H., Borne A., Kohanim S., Oh C.S., Mawlawi O., Kim E.E. (2007). Functional Imaging of Estrogen Receptors with Radiolabeled-GAP-EDL in Rabbit Endometriosis Model. Acad Radiol.
10 Dunselman G.A., Willebrand D., Land J.A., Bouckaert P.X., Evers J.L. (1989). A rabbit model of endometriosis. Gynecol Obstet Invest.